# [^18^F]-Labeled (R)-(2-(2-(2-methylpyrrolidin-1-yl)ethyl)benzofuran-5-yl)(4-fluorophenyl)-methanone

Chemical name: | [^18^F]-Labeled (R)-(2-(2-(2-methylpyrrolidin-1-yl)ethyl)benzofuran-5-yl)(4-fluorophenyl)-methanone | [image]
Abbreviated name: | [^18^F]9 | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | Histamine subtype-3 (H_3_) receptor | [image]
Target Category: | Receptors | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents; - Non-Human Primates | Structures of compound 12 and [^18^F]9 (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=H3%20receptor%20and%20imaging)]

[^18^F]-Labeled (R)-(2-(2-(2-methylpyrrolidin-1-yl)ethyl)benzofuran-5-yl)(4-fluorophenyl)-methanone, abbreviated as [^18^F]9, is a 2-aminoethylbenzofuran-based histamine subtype 3 receptor (H_3_R) antagonist/inverse agonist that was developed for imaging H_3_R with positron emission tomography (PET) (1).

H_3_R is one of the four G-protein–coupled receptors of the histamine receptor family. The human H_3_R gene is located on chromosome 20q13.33, and its products are expressed predominantly in the basal ganglia, hippocampus, and cortical areas, which participate in the synthesis and release of neurotransmitters (e.g., acetylcholine, dopamine, serotonin, and noradrenaline) from histaminergic neurons (2-4). Imbalance of the histaminergic interactions results in a number of pathological states, which might be treated with H_3_R ligands as neuronal system modulators (5). To date, a large class of H_3_R ligands has been reported, which is either imidazole or non-imidazole in structure (1). These ligands have been applied to correct sleep and wakefulness disorders and narcolepsy (6). H_3_R antagonists have also been considered to be useful in correcting cognitive disorders and memory processes (7). However, there are many challenges for H_3_R ligand development because of the complexity of the central histaminergic system, the diversity of actions, and the overlapping pharmacology of H_3_R- and H_4_R-targeting compounds (5).

H_3_R imaging with specific radioligands has the potential to elucidate changes in the distribution and density of H_3_R in living human brain and to determine the dose dependence of the extent and duration of H_3_R occupancy by candidates. In general, non-imidazole compounds appear more promising as radiotracers for H_3_R imaging. In an effort to develop an ^18^F-labeled H_3_R ligand, Bao et al. selected a new chemotype compound 9, a non-imidazole 2-aminoethylbenzofuran-based H_3_R antagonist/inverse agonist, for imaging feasibility evaluation in animals (1). Compound 9 has previously been shown to have a high affinity and selectivity for human H_3_R and to be able to cross the blood−brain barrier (8). In addition, compound 9 can be labeled with no-carrier-added fluorine-18 (t_1/2_ = 109.7 min) at an aryl carbon. The results obtained by Bao et al. have shown that [^18^F]9 is an effective radioligand for H_3_R imaging in mice and monkeys (1).

### Related Resource Links:

Nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=histamine%20H3%20receptor) and protein (http://www.ncbi.nlm.nih.gov/protein?term=histamine%20H3%20receptor) sequences of H_3_R

Bioassays (http://www.ncbi.nlm.nih.gov/pcassay?term=histamine%20H3%20receptor) of H_3_R in PubChem BioAssay

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=22313227)]

Compound 9 was prepared from commercially available (4-fluorophenyl)(4-hydroxyphenyl)methanone as described previously (1, 8). Bao et al. labeled compound 9 with cyclotron-produced [^18^F]fluoride ions through its nitro analog precursor 12 ((R)-(2-(2-(2-methylpyrrolidin-1-yl)ethyl)benzofuran-5-yl)(4-nitrophenyl)methanone) in a Synthia device equipped with a microwave heater (1). A higher decay-corrected radiochemical yield (RCY, 34%) of [^18^F]9 was obtained when the precursor 12 was reacted with [^18^F]fluoride ions in N,N-dimethylformamide than in MeCN (2%) or in dimethyl sulfoxide (6%). The reaction temperature (<90°C) was controlled by setting the microwave power between 50 W and 60 W because decomposition of [^18^F]9 became significant above 100°C. [^18^F]9 was separated with single-pass reverse-phase high-performance liquid chromatography (HPLC), with a high radiochemical purity (>99%). No residual precursor 12 or other chemical impurities were detected with HPLC in the formulated radioligand. The specific radioactivity of [^18^F]9 was 48.51 ± 8.18 GBq/µmol (1,311 ± 221 mCi/μmol; n = 12) at the time of intravenous injection to animals (~110 min from the end of radionuclide production). The average RCY of the formulated [^18^F]9 was 9.3 ± 5.8% (n = 12).

The distribution constant (log D_7.4_) value of [^18^F]9 between n-octanol and sodium phosphate buffer (0.15 M, pH 7.4) was 2.95 ± 0.06 (n = 6). The computed log D_7.4_ (pH 7.4) values of compounds 9 and 12 were 2.90 and 2.45, respectively. The computed partition coefficient (log P) values for compounds 9 and 12 were 4.79 ± 0.43 and 4.34 ± 0.34, respectively.

[^18^F]9 was found to be 98.8 ± 0.2% intact after 2.5 h in sodium phosphate buffer (pH 7.4) at room temperature (n = 6). [^18^F]9 was also stable in monkey whole blood (98.4 ± 0.07% intact; n = 6) and monkey plasma (99.2 ± 0.1% intact; n = 6) for 2.5 h at room temperature.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=22313227)]

Binding of compounds 9 and 12 to a group of human receptors was determined with competitive binding assays (no detailed description of the assays) (1). The assays confirmed the high H_3_R affinity of compound 9, with K_i_ in the nanomolar range (Table 1). The binding affinities of compound 9 for other human recombinant receptors and binding sites were at least 200-fold lower. The nitro precursor 12 had a binding affinity for human H_3_R almost 5-fold higher than that of compound 9 (Table 1).

Table 1. K_i_ values of compounds 9 and 12 as determined with competitive binding assays.

Receptor or binding site | K_i_ (nM)
Receptor or binding site | Compound 9 | Compound 12
H_1_R | 5,440 | 7,055
H_2_R | 1,708 | 923
H_3_R | 1.9 ± 0.23 | 0.4 ± 0.04
H_4_R | >10,000 | >10,000
5-HT_1A_ | 432 | >10,000
5-HT_1B_ | >10,000 | >10,000
5-HT_1D_ | 6,380 | 5,237
5-HT_2A_ | 2,718 | 1,355
5-HT_2B_ | 3,152 | >10,000
Dopamine active transporter | >10,000 | 137
Muscarinic acetylcholine receptor M_1_ (M_1_) | 3,266 | 931
M_2_ | 462 | 681
M_3_ | 204 | 512
M_4_ | 351 | 415
M_5_ | 437 | 336
All others* | >10,000 | >10,000

*5-HT_1E,2C,3,5A,6 and 7_, α_1A,1B,1D,2A,2B and 2C_, β_1–3_, D_1–5_, σ_1,2_, serotonin transporter, and norepinephrine transporter.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=22313227)]

Bao et al. first determined the time–activity curve of [^18^F]9 in the brain of wild-type FVB mice (1). Images were acquired at baseline ([^18^F]9 only; 2.7 ± 1.1 MBq (73 ± 29 μCi)) and after pretreatment (30 min before injection of [^18^F]9) with the selective high-affinity H_3_R inverse agonist ciproxifan (2.0 mg/kg), nitro precursor 12 (2.0 mg/kg), or ligand 9 itself (1.0 mg/kg) (n = 3–4 mice/group). Brain uptake of the radioactivity was expressed as standardized uptake value (SUV), where SUV = (% injected dose per cm^3^ brain) × (g body weight).

[^18^F]9 crossed the blood–brain barrier quickly, with peak whole-brain uptake of 3.36 SUV at ~6.5 min. The brain radioactivity then declined slowly to ~2.3 SUV by 90 min. In mice pretreated with ciproxifan, the brain radioactivity also quickly peaked, but at a lower level of ~1.98 SUV at 4.5 min after [^18^F]9 injection, and then reduced gradually to 1.09 SUV at 90 min. In mice pretreated with nitro precursor 12 or ligand 9, the [^18^F]9 brain radioactivity peaked at 3.5 min, with higher values of 4.34 SUV and 4.07 SUV, respectively. The brain radioactivity then decreased quickly to <1.20 SUV by 90 min. The brain radioactivity uptake was different between the pretreatment experiments with ciproxifan and those with the structural congeners 12 and 9. One possible explanation is that, at the administered doses, compounds 9 and 12 displace the structurally similar [^18^F]9 from plasma proteins, giving a higher plasma free fraction and greater entry of [^18^F]9 into brain than in the baseline experiments. Another possibility is that compounds 9 and 12, but not ciproxifan, blocks [^18^F]9 from binding to other unknown sites in the periphery, thereby increasing availability of [^18^F]9 for brain entry. Overall, these results indicate that a high proportion of brain radioactivity in the baseline experiments represented specific binding of [^18^F]9 to H_3_R.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=22313227)]

Bao et al. then determined the time–activity curve of [^18^F]9 in the brains of male rhesus monkeys at baseline ([^18^F]9 only; 144.67 ± 17.02 MBq (3.91 ± 0.46 mCi); n = 4 monkeys) and after pretreatment with ciproxifan (2.0 mg/kg; n = 3 of the four monkeys) or compound 9 (1.0 mg/kg; n = 2 of the four monkeys) 30 min before [^18^F]9 injection (1). PET scans were acquired for 180 min, except for one scan of 120 min. In two of the monkeys, arterial blood was sampled at every 15 s for an initial 2 min, followed by further sampling at 3, 5, 10, 30, 60, 75, 90, 120, 150, and 180 min after [^18^F]9 injection. The radioactivity in each region of the brain was expressed as SUV. The two-tissue compartment model was applied to calculate the total distribution volume (V_T_).

[^18^F]9 entered the brain tissue well, with peak uptake in H_3_R-rich regions, such as striatum (4.45 SUV at ~27.5 min) and frontal cortex (3.86 SUV at ~47.5 min). Peak radioactivity in other regions was lower, but still higher than in cerebellum (2.76 SUV). The radioactivity in all regions decreased slowly to the end of PET scans (180 min). There was no radioactivity uptake into the skull. These results showed that the distribution of [^18^F]9 reflected the distribution of H_3_R. Pretreatment with ciproxifan reduced the peak radioactivity in H_3_R-rich regions, such as frontal cortex and striatum, but not in cerebellum. Subsequent washout of radioactivity from all H_3_R-containing regions was slow. Pretreatment with compound 9 reduced peak radioactivity in all brain regions, where the radioactivity declined to a common low level at 180 min. The summed PET images from pretreatment experiments with compound 9 showed a uniform low distribution of radioactivity across brain. Again, there was no radioactivity in the skull. Ciproxifan is known to show species differences in H_3_R binding affinity, with affinity for human H_3_R (K_i_ = 63 nM) >100-fold lower than that for rat H_3_R (K_i_ = 0.51 nM). The binding affinity of ciproxifan for monkey H_3_R is unknown. There is a possibility that the affinity of ciproxifan for monkey H_3_R is similar to that for human H_3_R, which may account for incomplete blockade of the brain H_3_R at the administered dose.

In the baseline experiments, the [^18^F]9 radioactivity cleared rapidly from plasma until ~50 min after injection, when the low level of decay-corrected plasma radioactivity became almost constant. Similar plasma time–radioactivity curves were observed in monkeys pretreated with ciproxifan or compound 9. The plasma free fraction of [^18^F]9 was 2.08 ± 0.14% at baseline and 1.4 ± 0.1% in monkeys pretreated with compound 9.

The [^18^F]9 metabolites in the monkey plasma were analyzed after extraction of the radioactivity (95.3 ± 7.44%; n = 115) from plasma with acetonitrile (1). Radio-HPLC showed that the [^18^F]9 intact in plasma declined continuously, while three radiometabolites [^18^F]A–C emerged. These radiometabolites appeared to be less lipophilic than [^18^F]9 (t_R_ = 5.63 min), according to their shorter retention times during HPLC. The radiometabolites were also observed in the plasma of monkeys pretreated with ciproxifan. In monkeys pretreated with compound 9, intact [^18^F]9 decreased more quickly to become the minor component, and the least lipophilic radiometabolite [^18^F]A became the major component in plasma. The ability of the radiometabolites to penetrate the blood–brain barrier was unknown. Considering their lower lipophilicities, these radiometabolites may enter brain tissues less readily than [^18^F]9 and may be less troublesome for quantification of [^18^F]9 binding to H_3_R. The routes of [^18^F]9 metabolism and the identities of the radiometabolites were also unknown. The lack of radioactivity uptake in skull indicated that none of the radiometabolites of [^18^F]9 was the [^18^F]fluoride ion, and that radiodefluorination did not occur for [^18^F]9.

The brain time–activity curves in baseline monkey experiments with [^18^F]9 fitted well to both one-tissue and two-tissue (2TC) compartmental models (1). The F test showed that the 2TC model gave the best fit to acquired data (Table 2). On average, ciproxifan reduced the normalized total volume of distribution (V_T_) 26%–34%, and ligand 9 reduced V_T_ ~49%–58%, indicating that the majority of the radioactivity in H_3_R-rich regions of the brain represented specific binding of [^18^F]9 to H_3_R.

Table 2. Estimation of V_T_ from 2TC model in two monkeys.

Region | Monkey 1 V_T_ | | | Monkey 2 V_T_ | | | Mean decrease (%)
Region | Baseline | Ciproxifan | Cold 9 | Baseline | Ciproxifan | Cold 9 | Ciproxifan | Cold 9
Frontal cortex | 64.1 | 43.5 | 29.5 | 42.1 | 26.7 | 16.4 | –34 | –58
Striatum | 54.7 | 42.7 | 29.1 | 45.3 | 31.6 | 19.7 | –26 | –52
Hippocampus | 60.4 | 45.3 | 31.2 | 50.8 | 30.4 | 20.8 | –33 | –54
Thalamus | 53.7 | 40.8 | 29.9 | 49.9 | 29.4 | 19.4 | –33 | –53
Cerebellum | 42.0 | 33.5 | 24.8 | 28.5 | 19.6 | 12.0 | –26 | –49

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=22172395)]

No references are currently available.

## References

1 Bao X., Lu S., Liow J.S., Zoghbi S.S., Jenko K.J., Clark D.T., Gladding R.L., Innis R.B., Pike V.W. (2012). Radiosynthesis and evaluation of an (18)F-labeled positron emission tomography (PET) radioligand for brain histamine subtype-3 receptors based on a nonimidazole 2-aminoethylbenzofuran chemotype. J Med Chem.
2 Leurs R., Bakker R.A., Timmerman H., de Esch I.J. (2005). The histamine H3 receptor: from gene cloning to H3 receptor drugs. Nat Rev Drug Discov.
3 Strakhova M.I., Fox G.B., Carr T.L., Witte D.G., Vortherms T.A., Manelli A.M., Miller T.R., Yao B.B., Brioni J.D., Esbenshade T.A. (2008). Cloning and characterization of the monkey histamine H3 receptor isoforms. Eur J Pharmacol.
4 Chepkova A., Yanovsky E., Parmentier R., Ohtsu H., Haas H.L., Lin J.S., Sergeeva O.A. (2012). Histamine receptor expression, hippocampal plasticity and ammonia in histidine decarboxylase knockout mice. Cell Mol Neurobiol.
5 Tiligada E., Kyriakidis K., Chazot P.L., Passani M.B. (2011). Histamine pharmacology and new CNS drug targets. CNS Neurosci Ther.
6 Barbier A.J. (2007). andBradbury, M.J. Histaminergic control of sleep-wake cycles: recent therapeutic advances for sleep and wake disorders. CNS Neurol Disord Drug Targets.
7 Esbenshade T.A., Browman K.E., Bitner R.S., Strakhova M., Cowart M.D., Brioni J.D. (2008). The histamine H3 receptor: an attractive target for the treatment of cognitive disorders. Br J Pharmacol.
8 Cowart M., Faghih R., Curtis M.P., Gfesser G.A., Bennani Y.L., Black L.A., Pan L., Marsh K.C., Sullivan J.P., Esbenshade T.A., Fox G.B., Hancock A.A. (2005). 4-(2-[2-(2(R)-methylpyrrolidin-1-yl)ethyl]benzofuran-5-yl)benzonitrile and related 2-aminoethylbenzofuran H3 receptor antagonists potently enhance cognition and attention. J Med Chem.